# ^64^Cu-1,4,7,10-Tetraazacyclododecane-N,N',N'',N'''-tetraacetic acid-C-type atrial natriuretic factor

Chemical name: | ^64^Cu-1,4,7,10-Tetraazacyclododecane-N,N',N'',N'''-tetraacetic acid-C-type atrial natriuretic factor
Abbreviated name: | ^64^Cu-DOTA-C-ANF
Synonym: | ^64^Cu-C-ANF
Agent Category: | Polypeptides
Target: | Natriuretic peptide clearance receptor (NPR-C)
Target Category: | Receptors
Method of detection: | Positron emission tomography (PET)
Source of signal / contrast: | ^64^Cu
Activation: | No
Studies: | - In vitro; - Rodents | No structure is available.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D)]

The ^64^Cu-labeled 1,4,7,10-tetraazacyclododecane-N,N',N'',N'''-tetraacetic acid (DOTA)-C-type atrial natriuretic factor (C-ANF), abbreviated as ^64^Cu-DOTA-C-ANF, is a positron emission tomography (PET) tracer that has been developed by Liu et al. for imaging atherosclerotic lesions by targeting natriuretic peptide clearance receptor (NPR-C) overexpressed on the surface of endothelial cells and vascular smooth muscle cells (VSMCs) in response to vascular injury (1). C-ANF is a fragment of C-type natriuretic peptide (CNP). The half-life of ^64^Cu is 12.7 h (β^+^ = 17%, β^–^ = 40%).

The natriuretic peptides are a family of three structurally related but genetically distinct peptides (atrial natriuretic peptide (ANP), brain natriuretic peptide (BNP), and CNP) (2, 3). These peptides exert their biological effects (natriuretic, diuretic, and vasodilating) by binding to three distinct natriuretic peptide receptors (NPRs): NPR-A, NPR-B, and NPR-C (4-6). CNP was originally isolated as a 22-amino-acid peptide from the porcine brain and has been found in human vascular endothelial cells, myocardium, kidneys, reproductive organs, and other tissues (7, 8). CNP preferentially binds to NPR-B, which is more abundant in veins than in arteries. Activation of the CNP/NPR-B pathway increases cyclic guanosine monophosphate (cGMP) in VSMCs and mediates vasorelaxation (2, 5). Some effects of the CNP are mediated by NPR-C, which is abundantly expressed in endothelial cells and in vessel neointima after arterial injury, where CNP/NPR-C signaling is implicated in an anti-proliferative action on VSMCs and endothelial cells (9, 10). CNP may also contribute to the anti-mitogenic and vasodilatory effects of ANP and BNP. However, CNP lacks significant natriuretic or diuretic effects (6).

Because of the findings that CNP/NPR-C is highly expressed in the vessel neointima and VSMCs at the sites of atherosclerotic plaques, Liu et al. investigated the potential of C-ANF to longitudinally image the progression of atherosclerosis in a rabbit model with PET (1). C-ANF was conjugated to DOTA and labeled with ^64^Cu (^64^Cu-DOTA-C-ANF). The results obtained by Liu et al. suggest that ^64^Cu-DOTA-C-ANF is a promising candidate tracer for in vivo PET imaging of NPR-C on atherosclerotic plaques (1).

### Related Resource Links:

- MICAD chapters on imaging agents of atherosclerosis (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=atherosclerosis+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad)
- Protein information on natriuretic peptides (http://www.ncbi.nlm.nih.gov/protein?term=natriuretic%20peptide)
- Protein information on natriuretic peptide receptors (http://www.ncbi.nlm.nih.gov/protein?term=natriuretic%20peptide%20receptors)
- Articles of natriuretic peptides and natriuretic peptide receptors in OMIM (http://www.ncbi.nlm.nih.gov/omim?term=natriuretic%20peptide%20receptors%20and%20natriuretic%20peptides)
- Clinical trials with natriuretic peptides in ClinicalTrials.gov (http://clinicaltrials.gov/ct2/results?term=natriuretic+peptides)

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/20008978)]

The C-ANF peptide (rat ANF(4-23),des-Gln^18^,des-Ser^19^,des-Gly^20,22^,des-Leu^21^) is commercially available. Liu et al. first conjugated C-ANF to DOTA-N-hydroxysuccinimide ester to produce DOTA-C-ANF with a conjugation efficiency of >95% (1). The presence of one DOTA per peptide was confirmed with liquid chromatography–electrospray ionization mass spectrometry. The DOTA-C-ANF was then labeled with ^64^Cu in ammonium acetate buffer (pH 5.5) for 1 h at 43°C, with a yield of 78.5 ± 4.8%. The ^64^Cu-DOTA-C-ANF conjugate was purified with solid-phase extraction. The specific activity was 58.1 ± 3.6 MBq/nmol (1.57 ± 0.097 mCi/nmol), and the radiochemical purity was >98%.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/20008978)]

The stability of ^64^Cu-DOTA-C-ANF was studied after incubation in rabbit serum for 1 h at 37°C. Analysis showed that 97.7 ± 3.9% of the ^64^Cu-DOTA-C-ANF was intact, indicating that ^64^Cu-DOTA-C-ANF was stable in rabbit serum (1). No binding affinity data were reported.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/20008978)]

Liu et al. investigated the pharmacokinetics of ^64^Cu-DOTA-C-ANF in normal rabbits after intravenous injection in one ear of the rabbit, followed by measurements of the radioactivity in blood samples from the contralateral ear (n = 4 rabbits) (1). The blood curve showed that the activity was 0.22% injected dose per gram (ID/g) at 1 min, but this value decreased sharply to 0.10% ID/g at 2 min and declined slowly to 0.02% ID/g at 60 min after injection.

To image atherosclerotic plaque, Liu et al. induced atherosclerotic-like lesions in the right femoral artery of male New Zealand white rabbits with air desiccation, followed by angioplasty at a later time point (TP) (1). PET imaging with ^64^Cu-DOTA-C-ANF was performed separately at 4–6 weeks (TP 1) after the air desiccation–induced injury (n = 9 rabbits), at 3 weeks (TP 2) after the second injury (balloon overstretching–induced injury performed at 1 week after TP 1; n = 6 rabbits), and at 4 weeks (TP 3) after TP 2 (n = 4 rabbits). Accumulation of ^64^Cu-DOTA-C-ANF was calculated as standardized uptake values (SUVs) in three-dimensional regions of interest by averaging the activity concentration corrected for decay over the contained voxels (multiple image slices). SUVs were not corrected for partial-volume effects. PET images clearly showed uptake of ^64^Cu-DOTA-C-ANF at the site of induced atherosclerosis, different from non-injured control vessels over the 1-h scan. The highest uptake at the injury site was observed at TP 1 (SUV = 2.01 ± 0.36) and decreased at later TPs. The uptake of ^64^Cu-DOTA-C-ANF on the injured vessel was significantly higher than the uptake on the control artery (P < 0.05) and muscle (P < 0.005) at each TP. The injured artery/muscle SUV ratio reached the highest value at TP 1 (3.59 ± 0.94); the value decreased significantly (P < 0.05) at TP 2 and remained constant at TP 3. The injured artery/muscle SUV ratio was also significantly higher than the control artery/muscle SUV ratio at each TP (P < 0.05). There was no significant difference among the control artery/muscle ratios at the three TPs (P > 0.05).

Competitive receptor blocking studies were performed in one rabbit at TP 1 and in 3 rabbits at 1 week from TP 2 after co-injection of ^64^Cu-DOTA-C-ANF with unlabeled C-ANF peptide (C-ANF:^64^Cu-DOTA-C-ANF = 100:1 molar ratio) (1). PET imaging showed similar ^64^Cu-DOTA-C-ANF uptake on injured arteries and non-injured controls. The injured/control arteries SUV ratio (1.08 at TP 1 and 1.07 ± 0.06 at TP 2) was significantly lower than the ratio obtained in non-blocking studies (injected with ^64^Cu-DOTA-C-ANF alone) (2.14 at TP 1 and 1.42 ± 0.03 at TP 2) (P < 0.05). The injured artery/muscle SUV ratio at TP 2 reduced from 3.05 ± 0.19 in non-blocking studies to 2.13 ± 0.18 (P < 0.01). In contrast, the control artery/muscle ratio did not change significantly (2.19 ± 0.16 in non-blocking studies versus 2.00 ± 0.06 at TP 2; P > 0.05).

In previous studies, removal of arterial endothelium with air desiccation has been shown to result in recruitment of VSMCs and proliferation of neointima. As a response, CNP is synthesized by VSMCs and NPR-C is highly expressed concurrently on the cells to inhibit the growth. The PET imaging results obtained by Liu et al. were mirrored by the progression of the atherosclerotic lesions. Histology of the femoral artery obtained at TP 1 showed the formation of primary neointimal lesions comprising VSMCs, foam cells, and extracellular matrix at the injury site. Immunohistochemistry also showed high expression of NPR-C in the lesions. Consistent with the findings, both the SUV ratio and the injured artery/muscle SUV ratio in PET imaging reached the maximum at TP 1. With progression of the plaque (as observed at TP 2 and TP 3), the VSMC population and the NPR-C expression decreased significantly, which resulted in the decrease of ^64^Cu-DOTA-C-ANF uptake. Liu et al. concluded that ^64^Cu-DOTA-C-ANF will likely be of utility in assessing the development of atherosclerosis early and at neointimal injury, but of less utility as an atherosclerotic plaque progresses and becomes relatively acellular (1).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22%20SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28primate%20NOT%20human%29)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20human)]

No references are currently available.

## References

1 Liu Y., Abendschein D., Woodard G.E., Rossin R., McCommis K., Zheng J., Welch M.J., Woodard P.K. (2010). Molecular imaging of atherosclerotic plaque with (64)Cu-labeled natriuretic peptide and PET. J Nucl Med.
2 Potter, L.R., A.R. Yoder, D.R. Flora, L.K. Antos, and D.M. Dickey, Natriuretic peptides: their structures, receptors, physiologic functions and therapeutic applications. Handb Exp Pharmacol, 2009(191): p. 341-66.
3 Goetze J.P. (2010). Biosynthesis of cardiac natriuretic peptides. Results Probl Cell Differ.
4 Piechota M., Banach M., Jacon A., Rysz J. (2008). Natriuretic peptides in cardiovascular diseases. Cell Mol Biol Lett.
5 Rubattu S., Sciarretta S., Valenti V., Stanzione R., Volpe M. (2008). Natriuretic peptides: an update on bioactivity, potential therapeutic use, and implication in cardiovascular diseases. Am J Hypertens.
6 Woodard G.E., Rosado J.A. (2008). Natriuretic peptides in vascular physiology and pathology. Int Rev Cell Mol Biol.
7 Sandow S.L., Tare M. (2007). C-type natriuretic peptide: a new endothelium-derived hyperpolarizing factor?. Trends Pharmacol Sci.
8 Maack T. (2006). The broad homeostatic role of natriuretic peptides. Arq Bras Endocrinol Metabol.
9 Rose R.A., Giles W.R. (2008). Natriuretic peptide C receptor signalling in the heart and vasculature. J Physiol.
10 Rubattu, S., S. Sciarretta, A. Morriello, C. Calvieri, A. Battistoni, and M. Volpe, NPR-C: a component of the natriuretic peptide family with implications in human diseases. J Mol Med, 2010